# [^11^C](5R)-5-(Methoxymethyl)-3-[4-[(3R)-4,4,4-trifluoro-3-hydroxybutoxy]phenyl]-2-oxazolidinone

Chemical name: | [^11^C](5R)-5-(Methoxymethyl)-3-[4-[(3R)-4,4,4-trifluoro-3-hydroxybutoxy]phenyl]-2-oxazolidinone
Abbreviated name:
Synonym: | [^11^C]Befloxatone
Agent Category: | Compound
Target: | Monoamine oxidase A (MAO-A)
Target Category: | Enzyme inhibitor
Method of detection: | PET
Source of signal\contrast: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates | Click on the above structure for additional information in PubChem.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20Befloxatone)]

Monoamine oxidase (MAO) is a mitochondrial enzyme that inactivates dopamine, noradrenaline, and serotonin in the brain (1, 2). Two isoforms (A and B) of the enzyme have been identified. MAO-A preferentially oxidizes serotonin and noradrenaline, whereas MAO-B preferentially oxidizes phenethylamine. Dopamine is a substrate for both enzymes. MAO-A is predominately associated with depression and anxiety disorders, whereas MAO-B is predominately associated with neurodegenerative diseases, such as Parkinson’s disease (PD), as indicated by studies with specific MAO isoform inhibitors (3-5).

[^11^C]Harmine ([^11^C]HAR), a potent and selective MAO-A inhibitor, has been found to be a useful positron emission tomography (PET) imaging agent in the human brain. However, [^11^C]HAR is extensively metabolized in plasma (6). (5R)-5-(Methoxymethyl)-3-[4-[(3R)-4,4,4-trifluoro-3-hydroxybutoxy]phenyl]-2-oxazolidinone (befloxatone), an oxazolidinone derivative, is a potent, reversible, and competitive MAO-A inhibitor (7). [^11^C]Befloxatone is being developed as a next-generation PET agent for the non-invasive study of brain MAO-A distribution and concentration in patients with psychiatric and neurologic disorders as well as for PET imaging in the heart.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20Befloxatone%20and%20synthesis)]

Dolle et al. (8) reported synthesis of [^11^C]befloxatone by cyclization reaction of [^11^C]phosgene ([^11^C]COCl_2_) with (R)-1-methoxy-3-[[4-[(3R)-4,4,4-trifluoro-3-hydroxybutoxy]-phenyl]amino]-2-propanol in CH_2_Cl_2_, with a radiochemical yield of 90-95% (end of synthesis) after high-performance liquid chromatography purification. The total, decay-corrected, radiochemical yield was 27-50% based on [^11^C]CH_4_. Radiochemical purities were >99%, with a specific activity of 18.5-74.0 GBq/μmol (0.5-2.0 Ci/μmol) at the end of synthesis.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20Befloxatone%20and%20in%20vitro)]

Curet et al. (7) reported that befloxatone inhibited MAO-A selectively and competitively in human and rat brain, heart, liver, and duodenum homogenates with K_i_ values ranging from 1.9-3.6 nM for MAO-A and from 270-900 nM for MAO-B. The inhibition of MAO-A by befloxatone was time-dependent and fully reversible after dilution.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20Befloxatone%20and%20rodentia)]

Valette et al. (9) performed biodistribution studies in rats after injection of 1.85 MBq (0.05 mCi) [^11^C]befloxatone. However, radioactivity was reported only in the heart. The myocardial uptake increased from 3.4% injected dose (ID)/g at 15 min to 3.8% ID/g at 30 min. Pretreatment with clorgyline (a MAO-A inhibitor) inhibited the myocardial uptake by 85% at 15 and 30 min.

### Other Non-Primate Mammals

[PubMed]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20Befloxatone%20and%20%28primate%20not%20human%29)]

Bottlaender et al. (10) performed PET studies in four baboons and found rapid accumulation in the brain minutes after injection of 551 ± 70 MBq (14.9 ± 1.9 mCi) [^11^C]befloxatone. The accumulation of [^11^C]befloxatone showed high radioactivity in the thalamus, striatum, pons, and cortical structures (1.5-1.8%ID/100 ml of tissue), and lower in cerebellum (1.07%ID/100 ml). Distribution volumes (DV) were calculated using Logan graphic analysis with arterial input function. The brain regions with the highest DV were the frontal cortex (23.0), putamen (22.4), temporal cortex (21.5), and thalamus (20.2). The cerebellum had the lowest DV (9.7). Pretreatment with befloxatone (0.4 mg/kg) and moclobemide (a MAO-A inhibitor, 10 mg/kg) inhibited >95% of uptake in all brain regions, whereas lazabemide (0.5 mg/kg), a selective MAO-B inhibitor, showed little inhibition. [^11^C]Befloxatone brain radioactivity was displaced by administration of befloxatone (30 min after the tracer injection). The displacement of the tracer from its binding sites was dose-dependent, with an IC_50_ of 0.02 mg/kg for all studied regions. The fraction of unchanged [^11^C]befloxatone in the plasma was 78% at 30 min with one major hydrophilic metabolite.

Valette et al. (9) performed PET imaging of the chest of baboons after injection of 223-370 MBq (6-10 mCi) [^11^C]befloxatone. Administration of befloxatone after the tracer displaced 85% of cardiac radioactivity. B_max_ for the heart was found to be 208 ± 13 pmol/ml tissue. Inhalation of tobacco smoke decreased the cardiac B_max_ to 150 ± 6.2 pmol/ml (P = 0.03), whereas nicotine did not. Therefore, a single cigarette (unknown compounds) can interfere with the cardiac turnover of catecholamines. [^11^C]Befloxatone revealed a good visualization of the heart with 6%ID/100 ml at 20 min. Clearance of [^11^C]befloxatone radioactivity from the lung was rapid with a heart-to-lung ratio of 3.5 at 60 min.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20Befloxatone%20and%20human)]

No publication is currently available.

## References

1 Richards J.G. Saura J. Ulrich J. Da Prada M. Molecular neuroanatomy of monoamine oxidases in human brainstem Psychopharmacology (Berl) 1992 106SupplS21 3 1546134
2 Saura J., Kettler R., Da Prada M., Richards J.G. (1992). Quantitative enzyme radioautography with 3H-Ro 41-1049 and 3H-Ro 19-6327 in vitro: localization and abundance of MAO-A and MAO-B in rat CNS, peripheral organs, and human brain. J Neurosci.
3 Murphy D.L., Wyatt R.J. (1972). Reduced monoamine oxidase activity in blood platelets from schizophrenic patients. Nature.
4 Murphy D.L., Weiss R. (1972). Reduced monoamine oxidase activity in blood platelets from bipolar depressed patients. Am J Psychiatry.
5 Jarman J., Glover V., Sandler M., Turjanski N., Stern G. (1993). Platelet monoamine oxidase B activity in Parkinson's disease: a re-evaluation. J Neural Transm Park Dis Dement Sect.
6 Bergstrom M., Westerberg G., Langstrom B. (1997). 11C-harmine as a tracer for monoamine oxidase A (MAO-A): in vitro and in vivo studies. Nucl Med Biol.
7 Curet O., Damoiseau G., Aubin N., Sontag N., Rovei V., Jarreau F.X. (1996). Befloxatone, a new reversible and selective monoamine oxidase-A inhibitor. I. Biochemical profile. J Pharmacol Exp Ther.
8 Dolle F., Valette H., Bramoulle Y., Guenther I., Fuseau C., Coulon C., Lartizien C., Jegham S., George P., Curet O., Pinquier J.L., Bottlaender M. (2003). Synthesis and in vivo imaging properties of [11C]befloxatone: a novel highly potent positron emission tomography ligand for mono-amine oxidase-A. Bioorg Med Chem Lett.
9 Valette H., Bottlaender M., Dolle F., Coulon C., Ottaviani M., Syrota A. (2005). Acute inhibition of cardiac monoamine oxidase A after tobacco smoke inhalation: validation study of [11C]befloxatone in rats followed by a positron emission tomography application in baboons. J Pharmacol Exp Ther.
10 Bottlaender M., Dolle F., Guenther I., Roumenov D., Fuseau C., Bramoulle Y., Curet O., Jegham J., Pinquier J.L., George P., Valette H. (2003). Mapping the cerebral monoamine oxidase type A: positron emission tomography characterization of the reversible selective inhibitor [11C]befloxatone. J Pharmacol Exp Ther.